# Radioiodinated anti–TAG-72 CC49 (Fab’)_2_ antibody fragment

Chemical name: | Radioiodinated anti–TAG-72 CC49 (Fab’)_2_ antibody fragment
Abbreviated name: | ^131^I/^125^I-CC49 (Fab’)_2_
Synonym: | ^131^I-CC49 Ab, ^125^I-CC49
Agent Category: | (Fab’)_2_ antibody fragment
Target: | (Sialyl-Tn (STn)) TAG-72
Target Category: | Antibody to antigen binding
Method of detection: | Single-photon emission tomography (SPECT), planar gamma imaging
Source of signal: | ^131^I, ^125^I
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=144964805), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=21689921) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=ShowDetailView&TermToSearch=182875&ordinalpos=1&itool=EntrezSystem2.PEntrez.Gene.Gene_ResultsPanel.Gene_RVDocSum) for more information about TAG-72.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(mab+cc49+fragment)+OR+((fab)+2+CC49))]

Radioiodinated anti–TAG-72 CC49 (Fab’)_2_ antibody fragment (^131^I-CC49 (Fab’)_2_), which is formed by the conjugation of ^125^I/^131^I with an anti–tumor-associated glycoprotein 72 (TAG-72) (Fab’)_2_ antibody fragment, has been developed for gamma imaging of cancers that express TAG-72 (1-4). ^125^I has a physical half-life (t_½_) of 60 days, and ^131^I has a t_½_ of 8 days. Although both can be used for in vivo gamma imaging, ^125^I has a gamma energy that is too low and ^131^I has a gamma energy that is too high. Another radioiodine, ^123^I, is more ideal for single-photon emission tomography (SPECT) and planar gamma imaging.

The TAG-72 antigen was isolated from the LS-174T human colon cancer xenograft as a high molecular weight glycoprotein (molecular mass of 10^6^ Da) with mucin-like characteristics (5-8). It is expressed on a variety of human adenocarcinomas such as pancreatic, breast, colorectal, prostate, endometrial, and ovarian cancers. This antigen has also been shown to be shed into the serum of cancer patients (9). The murine monoclonal antibody B72.3 (MAb B72.3) against TAG-72 mucin was initially generated by immunization of mice with a membrane-enriched fraction of a human breast carcinoma (10). With the use of affinity-purified TAG-72 from LS-174T as an immunogen, CC49 and other anti–TAG-72 MAbs with higher affinity constants (K_a_) have been produced and characterized (5, 6, 10, 11). CC49 MAb appears to react with a unique disaccharide sialyl-Tn (STn) epitope on TAG-72 (12, 13).

Radiolabeled MAbs have been developed for both the diagnosis and treatment of tumors (14). Radiolabeled B72.3 and CC49 exhibit excellent tumor localization capabilities with potential diagnostic and therapeutic applications in the clinical setting (15, 16). Because of their relatively large size, intact radiolabeled MAbs tend to have unfavorable imaging kinetics, poor tumor penetration, and high potential for human anti-mouse antibody response (11, 17-19). One possible approach to minimize these problems is reducing intact antibodies to smaller antibody fragments such as F(ab’)_2_ and Fab’ (20). Another approach is the development of genetic engineering methods to obtain single-chain Fv constructs (scFv) and multivalent scFv constructs (11, 21, 22). The F(ab’)_2_ and Fab’ fragments can generally be prepared by simple enzymatic cleavage. Pepsin digestion of the intact IgG removes the antibody constant region and produces the F(ab’)_2_ fragment with bivalent antigen-binding capability and a molecular weight of 100,000 (14). Because of the smaller size, the F(ab’)_2_ fragment has a faster blood clearance and a better tumor penetration than the intact IgG (2, 23). The removal of the Fc portion during the enzymatic cleavage also reduces nonspecific binding of F(ab’)_2_ to Fc receptors. The in vitro and in vivo properties of radioiodinated CC49 (Fab’)_2_ fragments have been studied and compared to those of the single-chain Fv constructs (1-4, 24).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(mab+cc49+fragment)+OR+((fab)+2+CC49))+AND+synthesis)]

CC49 MAb IgG was developed by the immunization of mice with purified TAG-72 (4). CC49 IgG was purified from ascetic fluid obtained from immunized mice. CC49 (Fab’)_2_ was prepared by 2% pepsin digestion of the purified CC49 IgG at 37ºC for 16 h (1, 2). The digested fragments were dialyzed and purified using ion-exchange chromatography. Radioiodination of CC49 (Fab’)_2_ was performed with the use of 1,3,4,6-tetrachloro-3α,6α-diphenylglycoluril (IodoGen) as the oxidizing agent. Briefly, 100 μg of CC49 (Fab’)_2_ in 0.1 M sodium phosphate buffer (pH 7.2) was added to a glass tube coated with 20 μg IodoGen. Approximately 18.5 MBq (0.5 mCi) ^125^I-sodium iodide or ^131^I-sodium iodide was added and the mixture was incubated for 2 min at room temperature. Size-exclusion chromatography was performed immediately to purify the radiolabeled antibody. The labeling efficiency was 50%. SDS-PAGE analysis identified the ^125^I/^131^I-CC49 (Fab’)_2_ fragment molecular weight as ~100,000. The specific activity of ^125^I/^131^I-CC49 (Fab’)_2_ was ~111–185 kBq/μg (3–5 μCi/μg) or ~11.1–18.5 MBq/nmol (0.3–0.5 mCi/nmol) on the basis of the molecular weight of 100,000. Yokota et al. (2) reported a specific activity of 81.4–432.9 kBq/μg (2.2–11.7 μCi/μg) or 8.1–43.3 MBq/nmol (0.2–1.2 mCi/nmol). In another study, Yokota et al. (3) reported a radiochemical yield and purity of 30–50% with a specific activity of 0.34–0.4 MBq/μg (9.2–10.8 μCi/μg) or 34–40 MBq/nmol (0.9–1.1 mCi/nmol). Pavlinkova et al. (4) reported a specific activity of 111–333 kBq/μg (3–9 μCi/μg) or 11.1–33.3 MBq/nmol (0.3–0.9 mCi/nmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=((mab+cc49+fragment)+OR+((fab)+2+CC49)))]

The radioimmunoreactivity of ^125^I-CC49 (Fab’)_2_ was determined by a solid-phase radioimmunoassay using a TAG-72–positive extract of a LS-174T human colon carcinoma xenograft (1). ^125^I-CC49 was used as the competitor. The binding of ^125^I-CC49 (Fab’)_2_ was 39.1%, and the relative K_a_ was ~4 × 10^8^ M^–1^, which was similar to that of ^125^I-CC49 IgG. The binding of ^125^I-CC49 (Fab’)_2_ to purified TAG-72 was 22.1%. Yokota et al. (2) reported a binding of 35% to a TAG-72–positive extract. In another study, Yokota et al. (3) found >90% binding of purified ^125^I-CC49 (Fab’)_2_ to bovine submaxillary gland mucin (BSM)-coated beads. Pavlinkova et al. (4) used the surface plasmon resonance technique to measure the real-time interactions, and the investigators reported that the K_a_ of unlabeled CC49 (Fab’)_2_ was 1.04 × 10^8^ M−^1^ in binding to the immobilized BSM. In comparison, the K_a_ for the intact CC49 IgG was 1.14 × 10^8^ M−^1^. In the same study, the binding of ^125^I-CC49 (Fab’)_2_ to BSM was 81%.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=((mab+cc49+fragment)+OR+(fab)+2+CC49))+AND+rodentia)]

Biodistribution studies of ^125^I-CC49 (Fab’)_2_ were performed in nude mice bearing s.c. LS-174T human colon carcinomas (0.5–0.8 cm in diameter) on the back (1). The studies were conducted with i.v. administration of 0.278 MBq (7.5 μCi) ^125^I-CC49 (Fab’)_2_, and the mice were euthanized at various time points in groups (n = 3−4 in each group). The mean tumor radioactivity levels of ^125^I-CC49 (Fab’)_2_ in percent injected dose per gram (% ID/g) were 20.8 (6 h), 19.2 (24 h), 13.9 (48 h), and 9.1 (72 h) with the standard error of the mean (SEM) <15%. The mean liver radioactivity levels (% ID/g) were 6.7 (6 h), 11.1 (24 h), 5.3 (48 h), and 1.2 (72 h). The mean kidney radioactivity levels (% ID/g) were 15.8 (6 h), 2.2 (24 h), 0.8 (48 h), and 0.2 (72 h). The radiolocalization indexes (RI; ratios of % ID/g in tumor to % ID/g in normal tissue) of tumor/blood were 3.7 (6 h), 21.7 (24 h), 82.9 (48 h), and 277.0 (72 h). In comparison, the tumor/blood RIs for mice injected with ^131^I-CC49 IgG were 0.3 (4 h), 1.6 (24 h), and 4.1 (48 h). A separate pharmacokinetic study (n = 4 mice) showed that ^125^I-CC49 (Fab’)_2_ had a plasma clearance t_½α_ of 26 min and t_½β_ of 12 h, whereas ^131^I-CC49 IgG had a plasma clearance t_½α_ of 39 min and t_½β_ of 113 h. Gamma imaging of a mouse bearing the tumor with a dose of 1.85 MBq (50 μCi) ^131^I-CC49 (Fab’)_2_ clearly visualized the tumor at 30 h after injection (1). The bladder was also visualized. Yokota et al. (2) conducted microautoradiography studies of ^125^I-CC49 (Fab’)_2_ in mice bearing LS-174T tumors (0.5–1 cm diameter) with a dose of 0.56 MBq (15 μCi) or 6.8 μg (68 pmol). The autoradiography showed that CC49 (Fab’)_2_ gave a greater penetration of tumor than CC49 IgG. This greater penetration decreased after 24 h.

Pavlinkova et al. (4) performed dual-label studies by injecting 0.185 MBq (5 μCi) ^125^I-CC49 (Fab’)_2_ and 0.0925 MBq (2.5 μCi) ^131^I-CC49-(scFv)_2_ constructs simultaneously into nude mice (n = 6) bearing s.c. LS-174T tumors on the back. The mean tumor radioactivity levels (% ID/g) with <20% SEM were 14.63 (0.5 h), 12.48 (1 h), 25.82 (4 h), 35.74 (6 h), 28.06 (24 h), 19.42 (48 h), 13.11 (72 h), and 12.55 (120 h). The blood radioactivity levels were 30.15 (0.5 h), 27.88 (1 h), 16.32 (4 h), 10.09 (6 h), 1.68 (24 h), 0.36 (48 h), 0.16 (72 h), and 0.15 (120 h). The mean liver radioactivity levels were 7.47 (0.5 h), 6.79 (1 h), 7.84 (4 h), 6.03 (6 h), 2.24 (24 h), 1.21 (48 h), 1.21 (72 h), and 1.49 (120 h). The mean kidney radioactivity levels were 11.48 (0.5 h), 11.31 (1 h), 9.78 (4 h), 7.44 (6 h), 2.10 (24 h), 0.52 (48 h), 0.25 (72 h), and 0.23 (120 h). The RI of tumor/blood at 24 h was 16.7. In comparison, the RIs of tumor/blood for ^131^I-CC49 IgG and ^131^I-CC49 (scFv)_2_ were 3.4 and 80.3, respectively.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=((mab+cc49+fragment)+OR+(fab)+2+CC49))++AND+(dog+OR+rabbit+OR+pig+OR+sheep))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=((mab+cc49+fragment)+OR+(fab)+2+CC49))+AND+(primate+NOT+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=((mab+cc49+fragment)+OR+(fab)+2+CC49))+AND+human)]

No publication is currently available.

## References

1 Milenic D.E., Yokota T., Filpula D.R., Finkelman M.A., Dodd S.W., Wood J.F., Whitlow M., Snoy P., Schlom J. (1991). Construction, binding properties, metabolism, and tumor targeting of a single-chain Fv derived from the pancarcinoma monoclonal antibody CC49. Cancer Res.
2 Yokota T., Milenic D.E., Whitlow M., Schlom J. (1992). Rapid tumor penetration of a single-chain Fv and comparison with other immunoglobulin forms. Cancer Res.
3 Yokota T., Milenic D.E., Whitlow M., Wood J.F., Hubert S.L., Schlom J. (1993). Microautoradiographic analysis of the normal organ distribution of radioiodinated single-chain Fv and other immunoglobulin forms. Cancer Res.
4 Pavlinkova G., Beresford G.W., Booth B.J., Batra S.K., Colcher D. (1999). Pharmacokinetics and biodistribution of engineered single-chain antibody constructs of MAb CC49 in colon carcinoma xenografts. J Nucl Med.
5 Muraro R., Kuroki M., Wunderlich D., Poole D.J., Colcher D., Thor A., Greiner J.W., Simpson J.F., Molinolo A., Noguchi P., et al. (1988). Generation and characterization of B72.3 second generation monoclonal antibodies reactive with the tumor-associated glycoprotein 72 antigen. Cancer Res.
6 Johnson V.G., Schlom J., Paterson A.J., Bennett J., Magnani J.L., Colcher D. (1986). Analysis of a human tumor-associated glycoprotein (TAG-72) identified by monoclonal antibody B72.3. Cancer Res.
7 Katari R.S., Fernsten P.D., Schlom J. (1990). Characterization of the shed form of the human tumor-associated glycoprotein (TAG-72) from serous effusions of patients with different types of carcinomas. Cancer Res.
8 Xiao J., Horst S., Hinkle G., Cao X., Kocak E., Fang J., Young D., Khazaeli M., Agnese D., Sun D., Martin E. (2005). Pharmacokinetics and clinical evaluation of 125I-radiolabeled humanized CC49 monoclonal antibody (HuCC49deltaC(H)2) in recurrent and metastatic colorectal cancer patients. Cancer Biother Radiopharm.
9 Paterson A.J., Schlom J., Sears H.F., Bennett J., Colcher D. (1986). A radioimmunoassay for the detection of a human tumor-associated glycoprotein (TAG-72) using monoclonal antibody B72.3. Int J Cancer.
10 Colcher D., Hand P.H., Nuti M., Schlom J. (1981). A spectrum of monoclonal antibodies reactive with human mammary tumor cells. Proc Natl Acad Sci U S A.
11 Goel A., Baranowska-Kortylewicz J., Hinrichs S.H., Wisecarver J., Pavlinkova G., Augustine S., Colcher D., Booth B.J., Batra S.K. (2001). 99mTc-labeled divalent and tetravalent CC49 single-chain Fv's: novel imaging agents for rapid in vivo localization of human colon carcinoma. J Nucl Med.
12 Beresford G.W., Pavlinkova G., Booth B.J., Batra S.K., Colcher D. (1999). Binding characteristics and tumor targeting of a covalently linked divalent CC49 single-chain antibody. Int J Cancer.
13 Colcher D., Pavlinkova G., Beresford G., Booth B.J., Batra S.K. (1999). Single-chain antibodies in pancreatic cancer. Ann N Y Acad Sci.
14 Kowalsky R.J., Falen S.W. (2004). and Radiopharmaceuticals in nuclear pharmacy and nuclear medicine, American Pharmacists Association: Washington, D.C. p. 733-752.
15 Colcher D., Minelli M.F., Roselli M., Muraro R., Simpson-Milenic D., Schlom J. (1988). Radioimmunolocalization of human carcinoma xenografts with B72.3 second generation monoclonal antibodies. Cancer Res.
16 Colcher D., Esteban J., Carrasquillo J.A., Sugarbaker P., Reynolds J.C., Bryant G., Larson S.M., Schlom J. (1987). Complementation of intracavitary and intravenous administration of a monoclonal antibody (B72.3) in patients with carcinoma. Cancer Res.
17 Britton K.E. (1990). The development of new radiopharmaceuticals. Eur J Nucl Med.
18 Jain R.K. (1987). Transport of molecules across tumor vasculature. Cancer Metastasis Rev.
19 Primus F.J., Bennett S.J., Kim E.E., DeLand F.H., Zahn M.C., Goldenberg D.M. (1980). Circulating immune complexes in cancer patients receiving goat radiolocalizing antibodies to carcinoembryonic antigen. Cancer Res.
20 Behr T. Becker W. Hannappel E. Goldenberg D.M. Wolf F. Targeting of liver metastases of colorectal cancer with IgG, F(ab')2, and Fab' anti-carcinoembryonic antigen antibodies labeled with 99mTc: the role of metabolism and kinetics Cancer Res 1995 55Suppl23 5777s 5785s 7493346
21 Bird R.E., Hardman K.D., Jacobson J.W., Johnson S., Kaufman B.M., Lee S.M., Lee T., Pope S.H., Riordan G.S., Whitlow M. (1988). Single-chain antigen-binding proteins. Science.
22 Colcher D., Bird R., Roselli M., Hardman K.D., Johnson S., Pope S., Dodd S.W., Pantoliano M.W., Milenic D.E., Schlom J. (1990). In vivo tumor targeting of a recombinant single-chain antigen-binding protein. J Natl Cancer Inst.
23 Goldenberg D.M. (1993). Monoclonal antibodies in cancer detection and therapy. Am J Med.
24 Schott M.E., Frazier K.A., Pollock D.K., Verbanac K.M. (1993). Preparation, characterization, and in vivo biodistribution properties of synthetically cross-linked multivalent antitumor antibody fragments. Bioconjug Chem.